# ^99m^Tc(CO)_3_-Anti-vascular cell adhesion molecule-1 nanobody cAbVCAM1-5

Chemical name: | ^99m^Tc(CO)_3_-Anti-vascular cell adhesion molecule-1 nanobody cAbVCAM1-5
Abbreviated name: | ^99m^Tc-cAbVCAM1-5
Synonym:
Agent category: | Antibody fragment, nanobody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Adhesion molecule
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cAbVCAM1-5)]

Endothelial cells are important cells in inflammatory responses (1, 2). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space is highly orchestrated through various interactions with different adhesion molecules on endothelial cells (3).

VCAM-1 is found in very low amounts or is undetectable on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (4-8). VCAM-1 binds to very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression is also induced by oxidized low-density lipoproteins under atherogenic conditions (9). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. Microbubbles targeted with monoclonal antibody against VCAM-1 are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (10). Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chain camelid antibodies with efficient and specific tumor targeting (11-13). Broisat et al. (14) evaluated ten anti-VCAM-1 nanobodies, of which cAbVCAM1-5 was the lead nanobody. cAbVCAM1-5 is cross-reactive for human VCAM-1 (hVCAM1) and mouse VCAM-1 (mVCAM1) with nanomolar affinities. cAbVCAM1-5 was radiolabeled with ^99m^Tc using tricarbonyl chemistry (^99m^Tc-cAbVCAM1-5) for noninvasive in vivo single-photon emission computed tomography (SPECT) imaging of atherosclerotic lesions in apolipoprotein E (ApoE)-deficient (ApoE^–/–^) mice.

### Related Resource Links:

- Chapters in MICAD (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), cAbVCAM1-5 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=cAbVCAM1-5%20AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/gene/7412))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VCAM-1 (http://www.ncbi.nlm.nih.gov/omim/192225))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cAbVCAM1-5)]

cAbVCAM1-5 were produced as hexahistidine-tagged proteins in Escherichia coli (14). A solution of [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ and nanobody cAbVCAM1-5 (pH 7–8) was incubated for 90 min at 60°C, with a radiochemical purity of >95%. The specific activity and yield of ^99m^Tc-cAbVCAM1-5 were not reported. ^99m^Tc-cAbVCAM1-5 was >98% intact for up to 6 h at 20°C in phosphate-buffered saline (PBS). ^99m^Tc-cAbBcII10 was prepared similarly as a control.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cAbVCAM1-5%20and+in+vitro)]

Binding experiments with cAbVCAM1-5 with the use of a Biacore sensor chip immobilized with mVCAM1 or hVCAM1 protein were performed (14). The K_d_ values of cAbVCAM1-5 were calculated to be 2.0 nM and 6.5 nM for mVCAM1 and hVCAM1, respectively. cAbBcII10 showed no binding to mVCAM1 or hVCAM1.

Broisat et al. (14) performed cell uptake assays with ^99m^Tc-cAbVCAM1-5 (5 nmol) using mouse bEND5 endothelial cells. The assays were performed after incubation for 90 min at 37°C. High levels of radioactivity accumulated in bEND5 cells that were activated with TNFα compared to non-stimulated bEND5 cells (P < 0.05). Co-incubation with 500-fold excess unlabeled cAbVCAM1-5 almost completely inhibited the radioactivity in TNFα-activated bEND5 cells. Flow cytometry analysis also showed binding of cAbVCAM1-5 to TNFα-activated mouse and human endothelial cells, whereas cAbBcII10 showed no binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cAbVCAM1-5%20and+rodentia)]

Broisat et al. (14) performed ex vivo biodistribution studies in ApoE^–/–^ mice (n = 6/group) and control C57Bl/6J mice (n = 4/group) at 3 h after injection of ^99m^Tc-cAbVCAM1-5 or ^99m^Tc-cAbBcII10. The accumulation of both tracers was highest in the kidneys (>222% ID/g) in both types of mice. The VCAM-1–positive organs from the ApoE^–/–^ mice and the control mice, such as the spleen (9.2% versus 7.4% ID/g), thymus (1.7% versus 1.5% ID/g), and bone marrow (10.7% versus 7.9% ID/g), showed higher accumulation of ^99m^Tc-cAbVCAM1-5 than the control ^99m^Tc-cAbBcII10 (0.1–1.0% ID/g) (P < 0.05). ^99m^Tc-cAbVCAM1-5 accumulation in the spleen, bone marrow, lymph node, thymus, liver, heart, and aortic arch lesions was significantly blocked (P < 0.05) by co-injection of 100-fold excess unlabeled cAbVCAM1-5 in ApoE^–/–^ mice. The accumulation of ^99m^Tc-cAbVCAM1-5 correlated with the volume of the atherosclerotic lesions as measured with immunochemistry analysis (P < 0.001), whereas no correlation with ^99m^Tc-cAbBcII10 was found.

SPECT imaging at 3 h after injection showed that the aortic arch/blood ratio for ^99m^Tc-cAbVCAM1-5 was higher (P < 0.05) in ApoE^–/–^ mice (n = 6; 2.5 ± 0.2) than C57Bl/6J mice (n = 4; 1.2 ± 0.2), whereas little difference was observed with ^99m^Tc-cAbBcII10 (1.0 ± 0.2 versus 0.8 ± 0.1) (14). The aortic arch lesions, kidneys, and urinary bladder were clearly visualized in the ApoE^–/–^ mice. Co-injection of 100-fold excess unlabeled cAbVCAM1-5 abrogated the visualization of the lesions in the aortic arch but not the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cAbVCAM1-5%20and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cAbVCAM1-5%20and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cAbVCAM1-5%20and+human)]

No publication is currently available.

## References

1 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
2 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
3 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
4 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
5 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
6 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
7 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
8 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
9 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
10 Kaufmann B.A., Sanders J.M., Davis C., Xie A., Aldred P., Sarembock I.J., Lindner J.R. (2007). Molecular imaging of inflammation in atherosclerosis with targeted ultrasound detection of vascular cell adhesion molecule-1. Circulation.
11 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
12 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
13 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
14 Broisat A., Hernot S., Toczek J., De Vos J., Riou L.M., Martin S., Ahmadi M., Thielens N., Wernery U., Caveliers V., Muyldermans S., Lahoutte T., Fagret D., Ghezzi C., Devoogdt N. (2012). Nanobodies Targeting Mouse/Human VCAM1 for the Nuclear Imaging of Atherosclerotic Lesions. Circ Res.